# ^99m^Tc-Hydrazinonicotinamide/tricine-eighteen-nucleotide RIα mRNA antisense small interfering oligoribonucleotides

Chemical name: | ^99m^Tc-Hydrazinonicotinamide/tricine-eighteen-nucleotide RIα mRNA antisense small interfering oligoribonucleotides
Abbreviated name: | ^99m^Tc-HYNIC/tricine-18-nt-RIα-mRNA-AS siRNAs
Synonym: | ^99m^Tc-RNAs, ^99m^Tc-HYNIC-RNAs
Agent Category: | siRNA
Target: | RIα mRNA
Target Category: | Gene silencing by siRNA
Method of detection: | Gamma planar imaging and Single-Photon Emission Computed Tomography (SPECT)
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure of ^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-AS siRNAs, with 2’-0-methyl and phosphorothioate backbone.modifications. The HYNIC chelator and tricine coordination have not been established by experiments.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-RNA+OR+(Radiolabeling+small+RNA+with+technetium-99m)&WebEnv=0qU2SB3WRTJ9z4417UqRGxzflLgYOaq6Wo8rE-q8ObXJTee71Xtx1HtoxjZcVsn2Mn6Jf8ewl1PUnT%40264134F666D44B80_0161SID&WebEnvRq=1)]

^99m^Tc-Hydrazinonicotinamide/tricine-eighteen-nucleotide RIα mRNA antisense small interfering oligoribonucleotides (^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-AS siRNAs) were developed as an in vivo agent for gamma planar/single-photon emission computed tomography (SPECT) imaging of the siRNAs (1). The in vivo imaging of ^99m^Tc-HYNIC-18-nt-RIα mRNA-AS siRNAs allows non-invasive monitoring of delivery of the siRNAs to the targeted cancer cells.

Radiolabeled antisense (AS) oligonucleotides can be used to identify and image the presence of a particular mRNA in vivo (2). Some of the major obstacles in developing a clinically useful radiolabeled AS probe include nonspecific affinity, ribonuclease destruction of the RNA target, and the lack of a receptor-targeting ligand. Small interfering ribonucleic acids (siRNA) comprise a class of RNAs that are 21–22 nucleotides in length and are generated from double-stranded RNAs (3). Fire et al. (4) first discovered that siRNAs silenced gene expression. It appears that siRNAs can direct the degradation of target mRNAs and induce specific posttranscriptional gene silencing (1, 3). It is possible to design siRNA molecules and deliver them to specific targets to silence a particular gene of choice. To develop siRNAs as therapeutic agents, the ability to monitor their in vivo distribution and target delivery is important. Both bioluminescent and nuclear imaging methods have been studied, but the optical method measures siRNA only indirectly (5). On the other hand, siRNA can be radiolabeled for direct imaging in humans. Liu et al. (1) reported the first radiolabeling of an 18-nt siRNA with ^99m^Tc for visualizing cellular delivery and in vivo imaging in mice. The 18-nt siRNA was an AS (5'-GCG UGC CUC CUC ACU GGC) against the RIα sense (S) mRNA (5'-GCC AGU GAG GAG GCA CGC) of the type I regulatory subunit α of cAMP-dependent protein kinase A (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Radiolabeling%5BAll+Fields%5D+AND+small%5BAll+Fields%5D+AND+Radiolabeling+small+RNA+with+technetium-99m&WebEnv=0rCFsxKO-Sns7jBs80-oDS73fnYO-11CKTuBvI6UHZQfCSR77ZxYdyDd62Ubv1-wnk4nyFy)]

Liu et al. (1) described the radiolabeling of the 18-nt-RIα mRNA-AS siRNAs with ^99m^Tc via the S-acetyl N-hydroxysuccinimide (NHS)-hydrazinonicotinamide (HYNIC) and tricine as the coligand. NHS-HYNIC was synthesized from 6-chloronicotinic acid by a three-step reaction scheme as reported by Abrams et al. (7). The structure was confirmed by elemental analysis, proton nuclear magnetic resonance, and mass spectroscopy. The 18-nt-RIα mRNA-AS siRNAs were synthesized with uniform phosphorothioate backbones and 2'-O-methyl modifications for in vitro and in vivo stability (1, 8). The 2'-O-methyl modifications preserve the ribose sugar pucker and retain the canonical, right-handed, A-form helical geometry for siRNA activity. The modifications also increase the nuclease resistance of oligoribonucleotides and siRNA duplexes. NHS-HYNIC in dimethylformamide was added by drop-wise to the lyophilized RNAs dissolved in 5 μg/μl bicarbonate buffer (pH 8.5) in a final HYNIC/RNA molar ratio of 10/1. The reaction mixture was incubated at room temperature for 60 min to produce the HYNIC-RNA conjugate. The conjugate was purified by high-performance liquid chromatography (HPLC) before ^99m^Tc labeling. The authors suggested that the HYNIC chelator was attached to the 5' primary amino group via the alkyl linker. For radiolabeling, purified HYNIC-RNA was dissolved in bicarbonate buffer (pH 8.5) and reacted with tricine, stannous chloride, and ^99m^Tc-pertechnetate. The mixture was incubated at room temperature for 30 min. The final ^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-AS siRNA was purified by a P4 gel column chromatography. The radiolabeling efficiency was >60%, the radiochemical purity was >95%, and the specific activity was 20 GBq/μmol (0.54 Ci/μmol) or 3.7 MBq/μg (100 μCi/μg). The integrity of the ^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-AS siRNA was confirmed by an HPLC hybridization shift assay. Similar ^99m^Tc labeling was also used to obtain the radiolabeled sense RNA of ^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-S RNAs.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeling+small+RNA+with+technetium-99m)+&WebEnv=0gQ-Sq4lhIqXu1nUhBocUGV6mGIHxJrdY-bUQcIv-2AlzW8zaeQAMAdmJWZvrgxmg1hcSsc131H6vt%40264134F666D44B80_0161SID&WebEnvRq=1)]

The stability and integrity of ^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-AS siRNAs after 24 h incubation in ACHN human kidney cancer cell culture (high RIα mRNA expression) were confirmed by the HPLC hybridization shift assay (1). The assay also confirmed that the siRNAs preserved the potency to anneal to their complementary strands. In the cellular accumulation studies, ^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-AS siRNAs had increased uptake over 24 h. There were 3 × 10^5^ molecules of siRNA in 1 × 10^6^ cells. Microautoradiograms of cells showed ^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-AS siRNAs uniformly distributed throughout the cytoplasm and nucleus. Similar uptake and distribution patterns were observed with radiolabeled S RNA.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeling+small+RNA+with+technetium-99m)&WebEnv=0brBhGv2cBa6b73-z0c_o_am9CTdhNZBKq3Y60pr4RMPy2hcrkR31tTeYrXkOSUwMOFILOq4LU3LKs%40264134F666D44B80_0161SID&WebEnvRq=1)]

Biodistribution and imaging studies of ^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-AS siRNAs were performed in nude mice bearing s.c. ACHN human kidney cancer tumors (~1 cm diameter) (1). Each mouse received an i.v. dose of 3,700 kBq/μg (100 μCi/μg) ^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-AS siRNAs. At 4 h after injection, the tumors were clearly visualized. Other tissues were also visualized; the greatest signal intensity was in the abdomen. After 24 h, the intensity of radioactivity decreased throughout the whole body, and the tumor was still visualized. Similar images were also obtained with ^99m^Tc-S RNA. Biodistribution studies were conducted in mice at the end of the 24-h imaging. The radioactivity levels of ^99m^Tc-HYNIC/tricine-18-nt-RIα mRNA-AS siRNAs (n = 5) in percent injected dose/g (% ID/g) were 0.67 ± 0.07 (tumor), 0.07 ± 0.01 (blood), 0.18 ± 0.05 (muscle), 13.36 ± 5.10 (kidney), 8.13 ± 2.81 (liver), 0.38 ± 0.16 (lung), 0.16 ± 0.06 (stomach), and 2.46 ± 0.91 (large intestine). For the ^99m^Tc-S RNA, the radioactivity levels (% ID/g) were 0.76 ± 0.07 (tumor), 0.06 ± 0.02 (blood), 0.28 ± 0.44 (muscle), 26.54 ± 2.56 (kidney), 9.58 ± 2.96 (liver), 0.44 ± 0.05 (lung), 0.43 ± 0.21 (stomach), and 1.22 ± 0.43 (large intestine). The study estimated that the siRNAs were deliverable into tumor tissues at a magnitude of 7 ng/g tumor tissue when 1 μg siRNAs was injected. This localization pattern might translate into 7.2 × 10^11^ siRNA molecules/g tumor tissue (7,000 siRNAs/cell).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeling+small+RNA+with+technetium-99m)+AND+(dog+OR+rabbit+OR+pig+OR+sheep)&WebEnv=02GbT07ZqStwP4eWRsgYWa3ZEw6YjEWUOsgaoNff66GDTGIKo1C7w7mZ5ouRad_YVPmDp9T_E5fBTw%40264134F666D4)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeling+small+RNA+with+technetium-99m)+AND+(primate+NOT+human)&WebEnv=0FVDkFxRvV7b7hF9DUoK7Pkaqr2DAdzPS7wIhnq1YFqhS0dgaq35UB3Bw2WvOAGm2GE16r_Wy9pf-v%40264134F666D44B80_0161SID)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeling+small+RNA+with+technetium-99m)+AND+human&WebEnv=0wGlFwQJaR9bhZqYsiYTAr-dFBMX_1uwpYL14Zr4XZDnZrZt2QG5pRkPTd-gbrdiPMNOgR0tEIDhap%40264134F666D44B80_0161SID&WebEnvRq=1)]

No publication is currently available.

## References

1 Liu N., Ding H., Vanderheyden J.L., Zhu Z., Zhang Y. (2007). Radiolabeling small RNA with technetium-99m for visualizing cellular delivery and mouse biodistribution. Nucl Med Biol.
2 Gauchez A.S. (1999). A. Du Moulinet D'Hardemare, J. Lunardi, J.P. Vuillez, and D. Fagret, Potential use of radiolabeled antisense oligonucleotides in oncology. Anticancer Res.
3 Novina C.D., Sharp P.A. (2004). The RNAi revolution. Nature.
4 Fire A., Xu S., Montgomery M.K., Kostas S.A., Driver S.E., Mello C.C. (1998). Potent and specific genetic interference by double-stranded RNA in Caenorhabditis elegans. Nature.
5 Bartlett D.W., Davis M.E. (2006). Insights into the kinetics of siRNA-mediated gene silencing from live-cell and live-animal bioluminescent imaging. Nucleic Acids Res.
6 Zhang Y.M., Wang Y., Liu N., Zhu Z.H., Rusckowski M., Hnatowich D.J. (2001). In vitro investigations of tumor targeting with (99m)Tc-labeled antisense DNA. J Nucl Med.
7 Abrams M.J., Juweid M., tenKate C.I., Schwartz D.A., Hauser M.M., Gaul F.E., Fuccello A.J., Rubin R.H., Strauss H.W., Fischman A.J. (1990). Technetium-99m-human polyclonal IgG radiolabeled via the hydrazino nicotinamide derivative for imaging focal sites of infection in rats. J Nucl Med.
8 Kraynack B.A., Baker B.F. (2006). Small interfering RNAs containing full 2'-O-methylribonucleotide-modified sense strands display Argonaute2/eIF2C2-dependent activity. Rna.